# ^124^I-Labeled humanized CH2-domain-deleted anti-tumor-associated glycoprotein-72 (TAG-72) monoclonal antibody

Chemical name: | ^124^I-Labeled humanized CH2-domain-deleted anti-tumor-associated glycoprotein-72 (TAG-72) monoclonal antibody
Abbreviated name: | [^124^I]-HuCC49deltaC_H_2
Synonym:
Agent Category: | Antibody
Target: | Tumor-associated glycoprotein 72 (TAG-72)
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22SUBSTANCENAME%22%5BSubstance%5D%20AND%20Background%5BAll%20Fields%5D&cmd=DetailsSearch)]

Tumor-associated glycoprotein 72 (TAG-72) is a high molecular weight mucigenous protein that is found mainly in the extracellular matrix of neoplastic tumors (1). This glycoprotein is usually not expressed in normal tissues, but it is overexpressed in the tumors of several cancers, such as those of the colon and rectum (colorectal cancer), stomach, pancreas, ovaries, prostate, lung, breast, etc. Therefore, TAG-72 is considered to have a great deal of theranostic value (useful for the diagnosis and/or therapy of a disease) because it can be used for antigen-directed surgical resection of cancerous tumors with radiolabeled anti-TAG-72 monoclonal antibodies (mAb) (1). In addition, the detection or absence of TAG-72 expression in colorectal cancer tumors has been shown to have a prognostic value because individuals who had complete removal of tumors with surgery guided by mouse anti-TAG-72 mAb were shown to have a long-term survival advantage compared to patients who had incomplete removal of the lesions (2). In an effort to develop diagnostic agents that can be used for the rapid detection of tumors that overexpress TAG-72, investigators developed a ^125^I-labeled complimentary determining region–grafted humanized C_H_2-domain-deleted anti-TAG-72 mAb ([^125^I]-HuCC49deltaC_H_2) and showed that it can be used in preclinical (mouse model) and human clinical settings to detect xenograft colorectal cancer tumors positive for TAG-72 (3). In the human studies, the ^125^I-labeled mAb was used in conjunction with a hand-held gamma detection probe that assisted the surgeon to precisely locate and resect the tumor, which resulted in improved prognosis for the patient (4).

However, the main limitation of using ^125^I to develop a targeted tracer is that this radionuclide has a long half-life (~60 days) and is difficult to handle, store, and dispose from the hospital operating room (4). In addition, it is not the most suitable radionuclide for diagnostic imaging because it is a low-energy gamma emitter and generates low-quality images with scintigraphy. Therefore, as an alternative, investigators have used ^124^I to produce various types of imaging probes (small molecules, proteins antibodies, etc.) because it has a half-life of ~4 days, emits β particles that yield superior images with positron emission tomography (PET), and is easier to handle, store, and dispose. On the basis of this information, Zou et al. labeled HuCC49deltaC_H_2 with ^124^I ([^124^I]-HuCC49deltaC_H_2) and in a preliminary study evaluated the ^124^I-labeled mAb for the detection of LS174T (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-188&Template=cellBiology) colon adenocarcinoma cell xenograft tumors (that express high levels of TAG-72) with PET in nude mice (4).

### Related Resource Links

Tumor-associated glycoprotein-72 (TAG-72)–related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=TAG-72+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=TAG-72) related to TAG-72

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=20691066%5Buid%5D&cmd=DetailsSearch)]

The Iodogen method was used for the ^124^I labeling of HuCC49deltaC_H_2 conjugated to 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid as described by Zou et al. (4). The radiochemical yield of the labeled mAb was reported to be 98%. The radiochemical purity, specific activity, and stability of [^124^I]-HuCC49deltaC_H_2 was not reported. The tracer was filtered through a 0.22-micron filter for in vivo use.

For use as a control, a commercially available preparation of ^18^F-labeled fluorodeoxyglucose ([^18^F]-FDG; 200 MBq/mL (5.4 Ci/mL)) was used to detect the xenograft tumors in the animals (4)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=20691066%5Buid%5D&cmd=DetailsSearch)]

Slavin-Chiorini et al. reported that HuCC49deltaC_H_2 inhibited the binding of mouse CC49 (muCC49) and HuCC49 to the TAG-72 antigen (5). The relative affinity constants (K_d_) of HuCC49deltaC_H_2, HuCC49, and muCC49 were determined to be 5.1 nM, 2.1 nM, and 2.3 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-HuCC49deltaCH2%20rodentia&cmd=DetailsSearch)]

Zou et al. compared the use of [^124^I]-HuCC49deltaC_H_2 and [^18^F]-FDG to detect LS174T cell xenograft tumors in nude mice (4). Two mice were injected with 0.6 MBq (16.2 μCi) and 0.75 MBq (20.25 μCi) [^124^I]-HuCC49deltaC_H_2, respectively, through the tail vein. Another two mice were injected intraperitoneally with 1.4 MBq (~30 μCi) and 2.5 MBq (~68 μCi) [^124^I]-HuCC49deltaC_H_2, respectively. As a control, one mouse was injected with 7.4 MBq (~200 μCi) [^18^F]-FDG through the tail vein. PET images of animals (under anesthesia) injected with [^124^I]-HuCC49deltaC_H_2 were acquired at 1, 18, and 24 h postinjection (p.i.), and PET scans of the animal injected with [^18^F]-FDG were obtained at ~50 min p.i. as described by Zou et al. (4).

The tumors were visible only in images acquired from animals injected with [^124^I]-HuCC49deltaC_H_2 through the tail vein at 18 h and 24 h p.i (4). Radioactivity was also detected in the thyroid and the bladder of these mice. Similar results were obtained with mice injected intraperitoneally with the ^124^I-labeled mAb at 18 h and 24 h p.i., but these animals also showed a high level of radioactivity in the liver. Very little uptake of [^18^F]-FDG was observed in the tumor of the control animal injected with [^18^F]-FDG, and the radiolabeled compound was present mainly in the heart, the brown tissue on the posterior neck, kidneys, and the bladder of the mouse.

On the basis of this preliminary study, the investigators concluded that [^124^I]-HuCC49deltaC_H_2 can be used to detect neoplastic tumors that overexpress the TAG-72 antigen in rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-HuCC49deltaCH2%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=20691066%5buid%5d&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=20691066%5buid%5d&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

Studies presented in this chapter were supported in part by National Cancer Institute grant R01 CA120023.

## References

1 Povoski S.P., Hatzaras I.S., Mojzisik C.M., Martin E.W. (2011). Oncologic theranostics: recognition of this concept in antigen-directed cancer therapy for colorectal cancer with anti-TAG-72 monoclonal antibodies. Expert Rev Mol Diagn.
2 Povoski, S.P., I.S. Hatzaras, C.M. Mojzisik, M.W. Arnold, G.H. Hinkle, C.L. Hitchcock, D.C. Young, and E.W. Martin, Jr., Antigen-Directed Cancer Surgery for Primary Colorectal Cancer: 15-Year Survival Analysis. Ann Surg Oncol, 2011
3 Cheng, K.T., Radioiodinated anti-TAG-72 humanized CH2 domain-deleted antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
4 Zou P., Povoski S.P., Hall N.C., Carlton M.M., Hinkle G.H., Xu R.X., Mojzisik C.M., Johnson M.A., Knopp M.V., Martin E.W., Sun D. (2010). 124I-HuCC49deltaCH2 for TAG-72 antigen-directed positron emission tomography (PET) imaging of LS174T colon adenocarcinoma tumor implants in xenograft mice: preliminary results. World J Surg Oncol.
5 Slavin-Chiorini D.C., Kashmiri S.V., Lee H.S., Milenic D.E., Poole D.J., Bernon E., Schlom J., Hand P.H. (1997). A CDR-grafted (humanized) domain-deleted antitumor antibody. Cancer Biother Radiopharm.